# Radioiodinated T84.66 minibody

Chemical name: | Radioiodinated T84.66 minibody
Abbreviated name: | ^123/124^I-T84.66 minibody
Synonym:
Agent category: | Antibody fragment
Target: | Carcinoembryonic antigen (CEA)
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT), positron emission tomography (PET)
Source of signal\contrast: | ^123^I, ^124^I
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66+minibody)]

Carcinoembryonic antigen (CEA) was first identified from extracts of human colon adenocarcinoma (1) and fetal gut (2). It is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas and in certain inflammatory conditions such as inflammatory bowel disease (3, 4). CEA has a molecular weight of ~180 kDa, and it can be shed and detected in the serum (5). CEA expression is observed in patients with various carcinomas of the colon, lungs, thyroid, uterus, ovaries, pancreas, and medullary thyroid (6). Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (7, 8). ^99m^Tc-Arcitumomab, a murine anti-CEA mAb Fab’ fragment, was developed for use in single-photon emission computed tomography (SPECT) imaging of CEA expression.

Single-chain variable fragments (scFvs) of antibodies with a molecular mass of 25 kDa are cleared very rapidly from the circulation, but they exhibit poor tumor retention because they have a lower affinity than the parent antibody (9). On the other hand, bivalent antibody fragments possess more ideal tumor-targeting characteristics, including rapid tissue penetration, high target retention, and rapid blood clearance. The diabody fragment (a dimer of scFvs; molecular mass = 55 kDa) and the minibody fragment (a dimer of scFvs-C_H_3 with a linker comprising 18 amino acids; molecular mass = 80 kDa) of a murine/human chimeric anti-CEA T84.66 antibody have been evaluated for targeting in several tumor antigen systems with rapid tumor localization and high-contrast imaging (9, 10). In particular, murine/human chimeric anti-CEA T84.66 antibodies, which retain excellent CEA-binding properties (dissociation constant = 0.01–0.6 nM) (11-13), were developed as CEA imaging agents. A T84.66 minibody was radiolabeled with ^124^I and ^123^I for localization of CEA-positive tumors in mice and humans, respectively (14, 15).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20synthesis)]

The recombinant T84.66 minibody (1 mg) was labeled with 185–370 MBq (5–10 mCi) ^124^I or ^123^I in the presence of Iodogen (14, 15). ^123^I-T84.66 minibody was isolated with size-exclusion high-performance liquid chromatography (HPLC) with a radiolabeling efficiency of >90%. In contrast, ^124^I-T84.66 minibody had a labeling efficiency of 46%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20in%20vitro)]

Radioimmunoreactivity of ^123/124^I-T84.66 minibody for recombinant CEA was determined with size-exclusion HPLC analysis to be >90% (14, 15).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20rodentia)]

Sundaresan et al. (14) performed biodistribution studies of ^124^I-T84.66 minibody in nude mice (n = 5 mice/group) with the use of a LS174T human colon carcinoma or C6 rat glioma subcutaneous xenograft model. Data were obtained at 18 h after injection. Accumulation of the ^124^I-T84.66 minibody in the CEA-expressing LS174T tumor was 20.55 ± 2.74% injected dose (ID)/g, and accumulation in the CEA-negative C6 tumor was 1.87 ± 0.38% ID/g. The liver, heart, and kidney had lower levels of radioactivity (1.18–1.78% ID/g) than the LS174T tumor. The ex vivo LS174T/C6 ratio was 26.19 ± 11.16 (n = 5) at 18 h. Positron emission tomography with the ^124^I-T84.66 minibody showed specific localization to the CEA-positive tumor and relatively low activity elsewhere in the mice at 4 and 18 h. The LS174T/C6 ratios were 3.46 ± 0.72 (n = 8) at 4 h and 10.85 ± 2.03 (n = 8) at 18 h. Low radioactivity in the abdominal region resulted in high-contrast images at 18 h. CEA-Positive tumors ~3 mm in diameter could be detected. No blocking experiments were performed, but a control tumor was used. The ^124^I-T84.66 minibody tumor uptake (20.55% ID/g) at 18 h was similar to the ^111^In-DOTA-T84.66 minibody tumor uptake (24.47% ID/g) at 12 h (16). However, ^111^In-DOTA-T84.66 minibody exhibited a higher liver accumulation (25.97 ± 0.99% ID/g at 24 h) than ^124^I-T84.66 minibody (1.18% ID/g at 18 h).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In+T84.66+minibody+and%20human)]

Wong et al. (15) performed SPECT imaging studies in 10 patients with colorectal cancer. Each patient received 185–370 MBq (5–10 mCi) of ^123^I-T84.66 minibody by intravenous injection, followed by serial scans at 2–4 h, 18–24 h, and 48 h. Blood and urine were sampled over the next 48–72 h. Tumor imaging was observed in 7 of the 8 patients who did not receive neoadjuvant therapy before surgery. Two patients received neoadjuvant radiation and chemotherapy, which significantly reduced tumor size before surgery and minibody infusion. At surgery, a 2-mm tumor focus was observed in one patient, and the other patient had no observable tumor; ^123^I-T84.66 minibody tumor imaging was not used in either of these pretreated patients. Mean serum residence time of the minibody was 29.8 h (10.9–65.4 h). No drug-related adverse reactions were observed. None of the 10 patients showed significant immune responses to the minibody. However, the mean residence time of the minibody in patients is longer than the physical half-life of ^123^I (13 h). The authors plan to further evaluate the minibody biodistribution and pharmacokinetic properties by labeling it with a longer-lived radionuclide, such as ^111^In. The total body radiation dose estimate was 0.012 cGy/mCi.

## NIH Support

R24-CA92845, CA08748, CA86438, P01 CA43904, CA33572

## References

1 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
2 Krupey J., Gold P., Freedman S.O. (1967). Purification and characterization of carcinoembryonic antigens of the human digestive system. Nature.
3 Kowalsky, R.J., and S.W. Falen, Radiopharmaceuticals in nuclear pharmacy and nuclear medicine2004, American Pharmacists Association: Washington, D.C. p. 733-752.
4 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
5 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
6 Package Insert. CEA-Scan (Arcitumomab) for the preparation of Tc 99m Arcitumomab1999, Immunomedics, Inc. p. 1-15.
7 Kenanova V., Wu A.M. (2006). Tailoring antibodies for radionuclide delivery. Expert Opin Drug Deliv.
8 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
9 Wu A.M., Chen W., Raubitschek A., Williams L.E., Neumaier M., Fischer R., Hu S.Z., Odom-Maryon T., Wong J.Y., Shively J.E. (1996). Tumor localization of anti-CEA single-chain Fvs: improved targeting by non-covalent dimers. Immunotechnology.
10 Viti F., Tarli L., Giovannoni L., Zardi L., Neri D. (1999). Increased binding affinity and valence of recombinant antibody fragments lead to improved targeting of tumoral angiogenesis. Cancer Res.
11 Fagerstam L.G., Frostell-Karlsson A., Karlsson R., Persson B., Ronnberg I. (1992). Biospecific interaction analysis using surface plasmon resonance detection applied to kinetic, binding site and concentration analysis. J Chromatogr.
12 Hefta L.J., Neumaier M., Shively J.E. (1998). Kinetic and affinity constants of epitope specific anti-carcinoembryonic antigen (CEA) monoclonal antibodies for CEA and engineered CEA domain constructs. Immunotechnology.
13 Williams L.E., Wu A.M., Yazaki P.J., Liu A., Raubitschek A.A., Shively J.E., Wong J.Y. (2001). Numerical selection of optimal tumor imaging agents with application to engineered antibodies. Cancer Biother Radiopharm.
14 Sundaresan G., Yazaki P.J., Shively J.E., Finn R.D., Larson S.M., Raubitschek A.A., Williams L.E., Chatziioannou A.F., Gambhir S.S., Wu A.M. (2003). 124I-labeled engineered anti-CEA minibodies and diabodies allow high-contrast, antigen-specific small-animal PET imaging of xenografts in athymic mice. J Nucl Med.
15 Wong J.Y., Chu D.Z., Williams L.E., Yamauchi D.M., Ikle D.N., Kwok C.S., Liu A., Wilczynski S., Colcher D., Yazaki P.J., Shively J.E., Wu A.M., Raubitschek A.A. (2004). Pilot trial evaluating an 123I-labeled 80-kilodalton engineered anticarcinoembryonic antigen antibody fragment (cT84.66 minibody) in patients with colorectal cancer. Clin Cancer Res.
16 Yazaki P.J., Wu A.M., Tsai S.W., Williams L.E., Ikler D.N., Wong J.Y., Shively J.E., Raubitschek A.A. (2001). Tumor targeting of radiometal labeled anti-CEA recombinant T84.66 diabody and t84.66 minibody: comparison to radioiodinated fragments. Bioconjug Chem.